# [^111^In-Diethylenetriaminepentaacetic acid-Pro^1^,Tyr^4^]bombesin

Chemical name: | [^111^In-Diethylenetriaminepentaacetic acid-Pro^1^,Tyr^4^]bombesin
Abbreviated name: | [^111^In-DTPA-Pro^1^,Tyr^4^]BN
Synonym: | ^111^In-BN, ^111^In-BBN
Agent Category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRP-R)
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | [^111^In-DTPA-Pro^1^,Tyr^4^]BN. The ^111^In coordination configuration has not been established by experiments.. Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=55584176), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=2925&ordinalpos=5&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about BN and GRP.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Radiolabeled+Bombesin+analog+OR+(DTPA)-BN)]

[^111^In-Diethylenetriaminepentaacetic acid-Pro^1^,Tyr^4^]-bombesin ([^111^In-DTPA-Pro^1^,Tyr^4^]BN) is a peptide analog of the human gastrin-releasing peptide (GRP) conjugated with ^111^In, and it was developed for single-photon emission computed tomography (SPECT) imaging of tumors with overexpressed GRP receptors (GRP-R) (1-3). ^111^In is a gamma emitter with a physical half-life (t_½_) of 2.8 days.

The amphibian bombesin (BN or BBN), a peptide of 14 amino acids, is an analog of human GRP, a peptide of 27 amino acids, which binds to GRP-R with high affinity and specificity (4, 5). Both GRP and BN share an amidated C-terminus sequence homology of seven amino acids, -Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system (6, 7). They also act as potential growth factors for both normal and neoplastic tissues. Specific BN receptors (BN-R) have been identified in CNS and GI tissues and a number of tumor cell lines. The BN-R superfamily includes at least four different subtypes, namely the GRP-R subtype (BB2), the neuromedin B receptor subtype (BB1), the BB3 subtype, and the BB4 subtype (8). Overexpression of GRP-R in various human tumors (e.g., breast, prostate, lung, colon, ovarian, and pancreatic cancers) provides opportunities to image tumors with the use of specific molecular imaging agents designed to target the GRP-R (5, 9-12).

There have been varying degrees of success in the development of GRP-R–targeted radiopharmaceuticals for diagnostic or therapeutic applications (12). Various BN analogs have been labeled with ^99m^Tc and ^111^In for SPECT imaging (13, 14). Despite some concern about the possible tumor growth–stimulatory effect of BN, Breeman et al. (2) synthesized the BN-R agonist [^111^In-DTPA-Pro^1^,Tyr^4^]BN. The study reported that this agonist had a high specific localization in GRP-R–positive tissues and tumors. [^111^In-DTPA-Pro^1^,Tyr^4^]BN differs from native BN in that pGlu^1^ is replaced with DTPA-Pro^1^, and Leu^4^ with Tyr^4^. Breeman et al. (2) showed that this agonist was internalized by GRP-R–expressing cells, whereas the antagonist ([^111^In-DTPA-Tyr^5^,D-Phe^6^]BN(5-13)NHEt) was not.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeled+Bombesin+analog+OR+(DTPA)-BN)+AND+synthesis)]

[DTPA-Pro^1^,Tyr^4^]BN was synthesized using the solid-phase method using the Fmoc strategy and Rink amide resin (2). Coupling of DTPA to [Pro^1^,Tyr^4^]BN was performed using tributyl-DTPA anhydride as the acylating agent. Radiolabeling of [DTPA-Pro^1^,Tyr^4^]BN with ^111^In used the same procedure as described by Bakker et al. (15). A 40- to 70-molar excess of peptide over ^111^In was used. The peptide in 0.01–0.1 M acetic acid was mixed with ^111^In in 0.04–0.05 M hydrochloric acid. The reaction mixture was incubated at room temperature for 10 min. The labeling efficiency was >95% (2). The radiochemical purity was >95% after 2 h, and 88%–92% after 24 h. Breeman et al. (1) reported that the incorporation of ^111^In into [DTPA-Pro^1^,Tyr^4^]BN appeared to drop to <95% if the ratio of ^111^In radioactivity versus the [DTPA-Pro^1^,Tyr^4^]BN peptide exceeded 270 MBq ^111^In/nmol peptide (7.3 mCi/nmol). The study also reported that heating the reaction mixture of [DTPA-Pro^1^,Tyr^4^]BN and ^111^In at 100ºC for 25 min did not appear to change the labeling efficiency and properties of [^111^In-DTPA-Pro^1^,Tyr^4^]BN. The final specific activity was up to a level of 100–150 MBq/μg (2.70–4.05 mCi/μg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DTPA)-BN))+AND+(in+vitro))]

Breeman et al. (2) conducted BN-R binding studies with membrane preparations of 7315b prolactin-secreting rat pituitary tumor cells and used [^125^I-Tyr^4^]BN as the radioligand for binding displacement. The unlabeled [DTPA-Pro^1^,Tyr^4^]BN was confirmed as a BN-R agonist because it significantly stimulated prolactin secretion. In the binding study of displacing the binding of [^125^I-Tyr^4^]BN to 7315b cells, the 50% inhibition concentration (IC_50_) for unlabeled [DTPA-Pro^1^,Tyr^4^]BN was 8 nM. In comparison, the IC_50_ values for unlabeled [Tyr^4^]BN and antagonist [DTPA-Tyr^5^,D-Phe^6^]BN(5-13)NHEt were 1.6 and 11 nM, respectively. In another study, Breeman et al. (1) used membranes prepared from the GRP-R–positive AR42J rat pancreatic tumor cells with [^111^In-DTPA-Pro^1^,Tyr^4^]BN as the radoligand and unlabeled [Tyr^4^]BN as the competitor. The IC_50_ value for [Tyr^4^]BN was 1 nM.

Tumor cell internalization studies were conducted in both GRP-R–positive CA20948 and AR42J exocrine pancreas tumor cells (2). [^111^In-DTPA-Pro^1^,Tyr^4^]BN (~0.1 nM) was incubated with these cells for 1 h. Extrapolated from Figure 4 in Breeman et al. (2), the specific membrane-bound (total binding minus nonspecific binding) radioactivity levels (% total radioactivity/mg protein; 3–4 × n = 3) in the CA20948 cells were ~5.7% and ~15.0% at 5ºC and 37ºC, respectively. The % internalization levels of [^111^In-DTPA-Pro^1^,Tyr^4^]BN were ~2.6% and ~13.9% at 5ºC and 25ºC, respectively. In the AR42J cells, the values were much higher. The specific membrane binding levels were ~21.7% and ~77.4% at 5ºC and 37ºC, respectively. The internalization levels of [^111^In-DTPA-Pro^1^,Tyr^4^]BN were ~6.1% and ~73.0% at 5ºC and 25ºC, respectively. Addition of 0.1 μM [Tyr^4^]BN almost completely blocked the binding and internalization of radioactivity by these cells. In another study, Breeman et al. (1) reported similar high values for the CA20948 cells as those for the AR42J cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DTPA)-BN))+AND+(rodentia))]

Biodistribution studies of [^111^In-DTPA-Pro^1^,Tyr^4^]BN were performed in Buffalo rats (210–260 g) bearing the 7315b rat pituitary tumor on the back (2). The dose of [^111^In-DTPA-Pro^1^,Tyr^4^]BN for each rat was not reported. The rats were euthanized 24 hr after administration. The tumor radioactivity level in percentage injected dose per gram (% ID/g) was 0.048 ± 0.008 (n = 3). The tumor/blood ratio was 14 ± 4. This radioactivity level was reduced to 0.015 ± 0.004% ID/g with co-injection of 100 μg of unlableled [Tyr^4^]BN. The radioactivity levels (% ID/g) in other major organs were 0.0036 ± 0.0009 (blood), 0.0056 ± 0.0015 (lung), 0.51 ± 0.07 (kidney), 0.011 ± 0.003 (liver), 0.0063 ± 0.0025 (pituitary gland), 0.76 ± 0.03 (pancreas), 0.078 ± 0.003 (colon), 0.024 ± 0.002 (adrenal), and 0.002 ± 0.0003 (muscle). Gamma imaging of the rats showed accumulation of radioactivity in the kidneys and the liver. The tumor was also visualized. No signs of toxicity or discomfort were observed, and no macroscopic abnormalities were found at autopsy. In another study, Breeman et al. (1) performed biodistribution studies of [^111^In-DTPA-Pro^1^,Tyr^4^]BN in normal rats. The radioactivity levels (n = 3) in the highly GRP-R–positive pancreas was 0.9% ID/g. This binding was determined to be specific based on co-injection of 100 μg of [Tyr^4^]BN. The pancreas/blood ratio was 529. Other GRP-R–positive tissues with significant specific binding were the antrum, fundus, jejunum, colon, cecum, adrenals, and pituitary. In rats bearing the GRP-R–positive AR42J tumor, gamma imaging clearly visualized the kidneys and tumor at 24 h with a dose of 15 MBq/0.1 μg (0.41 mCi/0.1 μg) [^111^In-DTPA-Pro^1^,Tyr^4^]BN.

Breeman et al. (3) studied the biodistribution of different specific activities of [^111^In-DTPA-Pro^1^,Tyr^4^]BN (0.01, 0.025, 0.1, or 0.5 μg peptide labeled with 1.5 MBq (40.5 μCi) ^111^In) in normal Lewis rats (n = 3). The rats were euthanized 48 h after injection. The organ radioactivity levels were not significantly affected by different amounts of injected peptide. The radioactivity levels in the blood, liver, and kidney were not affected by co-injection of 100 μg [Tyr^4^]BN. The radioactivity levels in GRP-R–positive organs (pancreas, fundus, and adrenals) were inhibited by >90%, 80%, and 50%, respectively, with co-injection of 100 μg [Tyr^4^]BN. Optimum amounts of radioligand appeared to be 0.02–0.1 μg [^111^In-DTPA-Pro^1^,Tyr^4^]BN (or 10-50 pmol based on ~2 kDa molecular mass). In a time study of 4 MBq/0.1 μg (0.11 mCi/0.1 μg) administered dose at 4, 24, and 48 h in normal Lewis rats after injection, the results indicated that maximum radioactivity localization occurred at 4 h. The total and peptide-bound radioactivity levels in the cumulative urinary excretion up to 48 h were 70% and 35% ID, respectively. Dynamic gamma imaging confirmed the rapid radioactivity distribution and instant uptake in the kidneys. After 24 h, 70% ID was excreted in the urine, and the total body retention was 10% ID. Another study showed that when [Tyr^4^]BN was injected 30 min after the radioligand, it was completely ineffective in blocking radioactivity uptake in the GRP-R–positive tissues. When 2 MBq/0.1 μg (54 μCi/0.1 μg) [^111^In-DTPA-Pro^1^,Tyr^4^]BN was injected into WAGRIJ rats bearing the CC531 colon carcinoma in the liver, the tumor radioactivity level at 24 h was 0.10% ID/g, and 50% was specific. Lewis rats bearing the CA20948 pancreas tumor in the hind leg (n = 6) received a dose of 15 MBq/0.1 μg (0.41 mCi/0.1 μg) radioligand, and the tumor radioactivity level at 24 h was 0.17 ± 0.02% ID/g with 90% specific uptake. Gamma imaging visualized the kidneys, urinary bladder, and the tumor. The study also showed that the absolute radioactivity uptake in GRP-R–positive tissues was not affected by the rate of administration (bolus injection versus slow infusion over 4 min).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DTPA)-BN))+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DTPA)-BN))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DTPA)-BN))+AND+(humans))]

No publication is currently available.

## References

1 Breeman W.A., de Jong M., Erion J.L., Bugaj J.E., Srinivasan A., Bernard B.F., Kwekkeboom D.J., Visser T.J., Krenning E.P. (2002). Preclinical comparison of (111)In-labeled DTPA- or DOTA-bombesin analogs for receptor-targeted scintigraphy and radionuclide therapy. J Nucl Med.
2 Breeman W.A., Hofland L.J., de Jong M., Bernard B.F., Srinivasan A., Kwekkeboom D.J., Visser T.J., Krenning E.P. (1999). Evaluation of radiolabelled bombesin analogues for receptor-targeted scintigraphy and radiotherapy. Int J Cancer.
3 Breeman W.A., De Jong M., Bernard B.F., Kwekkeboom D.J., Srinivasan A., van der Pluijm M.E., Hofland L.J., Visser T.J., Krenning E.P. (1999). Pre-clinical evaluation of [(111)In-DTPA-Pro(1), Tyr(4)]bombesin, a new radioligand for bombesin-receptor scintigraphy. Int J Cancer.
4 Smith C.J., Gali H., Sieckman G.L., Higginbotham C., Volkert W.A., Hoffman T.J. (2003). Radiochemical investigations of (99m)Tc-N(3)S-X-BBN[7-14]NH(2): an in vitro/in vivo structure-activity relationship study where X = 0-, 3-, 5-, 8-, and 11-carbon tethering moieties. Bioconjug Chem.
5 Ma L., Yu P., Veerendra B., Rold T.L., Retzloff L., Prasanphanich A., Sieckman G., Hoffman T.J., Volkert W.A., Smith C.J. (2007). In Vitro and In Vivo Evaluation of Alexa Fluor 680-Bombesin[7-14]NH(2) Peptide Conjugate, a High-Affinity Fluorescent Probe with High Selectivity for the Gastrin-Releasing Peptide Receptor. Mol Imaging.
6 Mantey S., Frucht H., Coy D.H., Jensen R.T. (1993). Characterization of bombesin receptors using a novel, potent, radiolabeled antagonist that distinguishes bombesin receptor subtypes. Mol Pharmacol.
7 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
8 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
9 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
10 Biddlecombe G.B., Rogers B.E., de Visser M., Parry J.J., de Jong M., Erion J.L., Lewis J.S. (2007). Molecular imaging of gastrin-releasing peptide receptor-positive tumors in mice using 64Cu- and 86Y-DOTA-(Pro1,Tyr4)-bombesin(1-14). Bioconjug Chem.
11 Nock B., Nikolopoulou A., Chiotellis E., Loudos G., Maintas D., Reubi J.C., Maina T. (2003). [99mTc]Demobesin 1, a novel potent bombesin analogue for GRP receptor-targeted tumour imaging. Eur J Nucl Med Mol Imaging.
12 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
13. de Visser, M., H.F. Bernard, J.L. Erion, M.A. Schmidt, A. Srinivasan, B. Waser, J.C. Reubi, E.P. Krenning, and M. de Jong, Novel (111)In-labelled bombesin analogues for molecular imaging of prostate tumours. Eur J Nucl Med Mol Imaging, 2007.
14 Ferro-Flores G., Arteaga de Murphy C., Rodriguez-Cortes J., Pedraza-Lopez M., Ramirez-Iglesias M.T. (2006). Preparation and evaluation of 99mTc-EDDA/HYNIC-[Lys 3]-bombesin for imaging gastrin-releasing peptide receptor-positive tumours. Nucl Med Commun.
15 Bakker W.H., Albert R., Bruns C., Breeman W.A., Hofland L.J., Marbach P., Pless J., Pralet D., Stolz B., Koper J.W., et al. (1991). [111In-DTPA-D-Phe1]-octreotide, a potential radiopharmaceutical for imaging of somatostatin receptor-positive tumors: synthesis, radiolabeling and in vitro validation. Life Sci.